# ^44^Sc-Labeled 1,4,7,10-tetraazacyclododecane-1,4,7,10-tetraacetic acid–conjugated puromycin

Chemical name: | ^44^Sc-Labeled 1,4,7,10-tetraazacyclododecane-1,4,7,10-tetraacetic acid–conjugated puromycin
Abbreviated name: | [^44^Sc]-DOTA-Pur
Synonym:
Agent Category: | Compound
Target: | Ribosomes (prokaryotic and eukaryotic)
Target Category: | Other (ribonucleoprotein)
Method of detection: | Positron emission tomography (PET)
Source of signal / contrast: | ^44^Sc
Activation: | No
Studies: | - In vitro; - Rodents | Structure not available in PubChem (http://www.ncbi.nlm.nih.gov/pcsubstance).

## Background

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed?term=Puromycin&cmd=DetailsSearch)]

Puromycin (http://www.sigmaaldrich.com/catalog/product/sigma/p9620?lang=en&region=US) (Pur) is an aminonucleoside antibiotic isolated from the bacteria Streptomyces alboniger. This antibiotic is a structural analog of aminoacyl-tRNA, and the insertion of Pur at the C-terminus of the protein inhibits further elongation of the protein chain in the ribosomes (at the translational level) in all organisms (prokaryotic and eukaryotic) (1). This phenomenon leads to accumulation of truncated and mis-folded proteins and culminates in cell death. The exact mechanism of action of Pur has been discussed by Starck and Roberts (2). Because cells in cancerous tumors have a very high rate of protein synthesis compared with normal cells, amino acids labeled with radionuclides have often been used to monitor anti-cancer therapy. The amino acids, however, can be utilized in the cells for protein synthesis through several different pathways; as a result, observations made with these tracers may not represent the actual anti-cancer efficacy of a drug (3). Protein synthesis is controlled primarily at the translation level, and it has been suggested that imaging the synthesis of nascent proteins may help researchers understand the relationships between the various normal and abnormal (diseased) physiological pathways in vivo (4). In this regard, fluorescence-labeled deoxy-cytidine derivatives of Pur and other fluorescent dyes have been used to investigate the synthesis of proteins in cells (5) and in cell-free systems (6), respectively. However, this approach has limited application under in vivo conditions because fluorescence cannot penetrate deep tissues and generates very low signal/noise ratios (4). Investigators have also used anti-Pur antibodies to study protein synthesis in the cell, but these reagents are most suited for use with immunoblots and produce inconsistent results at the cellular level (4).

In an effort to improve the visualization of protein synthesis under in vivo conditions, a 1,4,7,10-tetraazacyclododecane-1,4,7,10-tetraacetic acid (DOTA)-labeled derivative of Pur was prepared for labeling with radionuclides such as ^68^Ga or ^44^Sc, which can be used with positron emission tomography (PET) (7). Although ^68^Ga is useful in some clinical applications, the short half-life of this radionuclide (half-life = ~68 min) limits its use to the imaging of only those biological processes that occur rapidly (7). Because protein synthesis is a slow process, it requires the use of a tracer that has a longer half-life, such as ^44^Sc (half-life = ~4 h) (7). Eigner et al. labeled DOTA-Pur with ^44^Sc ([^44^Sc]-DOTA-Pur) and evaluated the use of this radiolabeled antibiotic for the visualization of AT1 cell tumors (derived from rat prostate carcinoma) and Walker carcinoma 256 cell tumors (rat breast carcinoma cell line) in rats (7). The biodistribution of [^44^Sc]-DOTA-Pur was also studied in these animals (7).

### Related Resource Links

Clinical trials (http://clinicaltrials.gov/ct2/results?term=Protein+synthesis&Search=Search) related to protein synthesis

Ribosomes (http://www.ncbi.nlm.nih.gov/omim?term=ribosomes) in Online Mendelian Inheritance in Man database (OMIM)

Ribosome structure (http://www.ncbi.nlm.nih.gov/pubmed?term=ribosome%20structure&cmd=DetailsSearch) in PubMed

## Synthesis

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed?term=DOTA-Pur&cmd=DetailsSearch)]

DOTA-Pur was synthesized and labeled with ^44^Sc as described by Eigner et al. (7). The radiochemical yield of [^44^Sc]-DOTA-Pur was 59.0 ± 6.0%, with a radiochemical purity of >97% as determined with thin-layer chromatography. The specific activity of purified [^44^Sc]-DOTA-Pur was 1.5 ± 0.1 GBq/μmol (40.5 ± 2.7 mCi/μmol). Purified [^44^Sc]-DOTA-Pur was formulated in 0.9% sodium chloride at a concentration of 30 MBq/ml (810 μCi/ml).

## In Vitro Studies: Testing in Cells and Tissues

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed?term=DOTA-Pur%20in%20vitro&cmd=DetailsSearch)]

The uptake of [^44^Sc]-DOTA-Pur was investigated in DU145 cells (http://www.atcc.org/ATCCAdvancedCatalogSearch/ProductDetails/tabid/452/Default.aspx?ATCCNum=HTB-81&Template=cellBiology) and BJ cells (http://www.atcc.org/ATCCAdvancedCatalogSearch/ProductDetails/tabid/452/Default.aspx?ATCCNum=CRL-2522&Template=cellBiology) in the presence or absence of increasing concentrations (10 pmol to ≥200 pmol) of either Pur (irreversible competitive inhibitor) or cyclohexamide (non-competitive inhibitor of Pur), as described elsewhere (7). The uptake of radioactivity by the DU145 cells and BJ cells in the absence of any inhibitor was 2.0 ± 0.1% of the applied dose per 1 × 10^6^ cells and 0.2 ± 0.1% of the applied dose per 1 × 10^6^ cells, respectively. Both cell lines were reported to incorporate 93% of the applied dose of radioactivity into the protein fraction (7).

In another study, unlabeled Pur (≥200 pmol) was shown to decrease the accumulation of label from [^44^Sc]-DOTA-Pur in the DU145 cells to <8.2 ± 0.2% of the initial uptake value (without Pur). Similarly, unlabeled cyclohexamide (≥200 pmol) decreased the incorporation of radioactivity in these cells to <12.1 ± 0.2% of the initial uptake value (7).

## Animal Studies

### Rodents

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed?term=DOTA-Pur%20rodentia&cmd=DetailsSearch)]

The biodistribution of [^44^Sc]-DOTA-Pur was investigated in rats bearing either AT1 cell or Walker carcinoma 256 cell tumors (7). The animals (number of animals not mentioned) were injected with a bolus of 20–25 MBq (540–675 μCi) [^44^Sc]-DOTA-Pur through the tail vein, and microPET dynamic images of the rodents were acquired for up to 120 min postinjection (p.i.). Both types of tumors showed the highest uptake of radioactivity and were clearly visible in the images between 3 min p.i. and 6 min p.i. The tumor/background ratios for both types of lesions were determined to be ≥40. High amounts of label were also detected in the kidneys and the bladder of the animals (exact data not presented), indicating that the tracer was excreted from the body mainly through the renal route (7). No blocking studies were reported.

After completion of the PET scans, the animals were euthanized at 2 h p.i. and 4 h p.i., and all the major organs were retrieved to determine the amount of radioactivity that accumulated in the various tissues (7). Low uptake of label was observed in the normal tissues of the animals (data not presented). The tumor/non-tumor tissue ratios were reported to be 6 and 9 at 2 h p.i. and 4 h p.i., respectively (7).

From these studies, the investigators concluded that [^44^Sc]-DOTA-Pur can probably be used for the imaging of ribosomal activity or protein synthesis in rodents (7).

### Other Non-Primate Mammals

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed?term=DOTA-Pur%20Other%20Non-Primate%20Mammals&cmd=DetailsSearch)]

No publication is currently available.

### Non-Human Primates

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed?term=DOTA-Pur%20Non-Human%20Primates&cmd=DetailsSearch)]

No publication is currently available.

## Human Studies

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed?term=DOTA-Pur%20Human%20Studies&cmd=DetailsSearch)]

No publication is currently available.

## Supplemental Information

[Disclaimers]

No information is currently available.

## References

1 Croons V., Martinet W., Herman A.G., De Meyer G.R. (2008). Differential effect of the protein synthesis inhibitors puromycin and cycloheximide on vascular smooth muscle cell viability. J Pharmacol Exp Ther.
2 Starck S.R., Roberts R.W. (2002). Puromycin oligonucleotides reveal steric restrictions for ribosome entry and multiple modes of translation inhibition. RNA.
3 Haubner R. (2010). PET radiopharmaceuticals in radiation treatment planning - synthesis and biological characteristics. Radiother Oncol.
4 Liu J., Xu Y., Stoleru D., Salic A. (2012). Imaging protein synthesis in cells and tissues with an alkyne analog of puromycin. Proc Natl Acad Sci U S A.
5 Starck S.R., Green H.M., Alberola-Ila J., Roberts R.W. (2004). A general approach to detect protein expression in vivo using fluorescent puromycin conjugates. Chem Biol.
6 Blower M.D., Feric E., Weis K., Heald R. (2007). Genome-wide analysis demonstrates conserved localization of messenger RNAs to mitotic microtubules. J Cell Biol.
7 Eigner S., Vera D.R., Fellner M., Loktionova N.S., Piel M., Lebeda O., Rosch F., Ross T.L., Henke K.E. (2013). Imaging of Protein Synthesis: In Vitro and In Vivo Evaluation of (44)Sc-DOTA-Puromycin. Mol Imaging Biol.